# ^99m^Tc-ethylenediamine N,N’-diacetic acid/hydrazinonicotinamide-Tyr^3^-octreotide

Chemical name: | ^99m^Tc-ethylenediamine N,N’-diacetic acid/hydrazinonicotinamide-Tyr^3^-octreotide
Abbreviated name: | ^99m^Tc-HYNIC-TOC
Synonym: | ^99m^Tc-EDDA/HYNIC-TOC
Agent Category: | Compound
Target: | Somatostatin receptor
Target Category: | Receptor-ligand binding
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Structure of ^99m^Tc-HYNIC-TOC.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc-HYNIC-TOC)]

Somatostatin (SS) is a cyclic peptide that is primarily expressed in the central nervous system and some peripheral tissues (1). Receptors for SS have been identified in the central nervous system, cells of neuroendocrine origin, the gastrointestinal tract, and even in lymphocytes (2). The SS receptor has a seven-transmembrane domain structure and belongs to the G-protein–coupled receptor family. Five subtypes of the SS receptor have been identified, and each subtype is produced from a single gene located on a different chromosome. This indicates tissue-specific regulation of SS receptor expression and suggests that each subtype has a distinct function in the various organs (2). Because of its several physiological functions, SS is considered to be a neurotransmitter or a hormone that acts through the autocrine and paracrine processes (3). In general, SS inhibits the production of hormones from various glands. SS has been evaluated for the treatment of various diseases, including cancers of endocrine origin as a result of hyperactive glands. However, SS has a short plasma half-life because of rapid enzymatic degradation and has been observed to be ineffective for such therapy (2). The development of SS analogs resistant to enzymatic degradation, but with a biological activity similar to SS, led to the application of these analogs for the treatment of cancerous tumors (4, 5).

The mechanism by which SS and its analogs inhibit tumor growth was detailed by Moody et al. (6). A cyclic octapeptide SS analog, octreotide, was synthesized and conjugated with diethylenetriamine pentaacetic acid (DTPA) for chelating radioactive indium (^111^In) to obtain ^111^In-DPTA-octreotide (^111^In-DPTA-OCT). On binding to the SS receptor, ^111^In-DPTA-OCT is rapidly internalized and results in accumulation of the radiochemical in the tumor cells. Subsequently, the tumors can be detected by scintigraphy and treated with radiolabeled peptides (6). Although ^111^In-DPTA-OCT is considered suitable for the detection and diagnosis of tumors bearing SS receptors, the use of ^111^In as a radionuclide has some limitations. This radioelement has limited availability, a long physical half-life (67 h), high gamma energy that results in increased radiation exposure of the patient, and suboptimal image characteristics (7, 8). Therefore, Decristoforo et al. used radioactive technetium (^99m^Tc) with a half-life of 6 h to generate ^99m^Tc-labeled hydrazinonicotinamide-Tyr^3^-octreotide (^99m^Tc-HYNIC-TOC), a radiochemical with superior imaging properties compared to ^111^In-DPTA-octreotide (9). This chapter describes the synthesis, in vitro and in vivo, and clinical studies performed with ^99m^Tc-HYNIC-TOC.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+HYNIC+TOC+synthesis)]

The synthesis of Tyr^3^-octreotide (TOC) has been described elsewhere (9-11). TOC and Lys^5^(butoxycarbonyl)-TOC (Lys^5^(BOC)-TOC) were purchased commercially. For the synthesis of HYNIC-TOC, 6-butoxycarbonyl-HYNIC, O-(7-azabenzotriazolyl)-1,1,3,3-tetramethyl-uronium hexafluorophosphate, and diisopropylethylamine dissolved in dimethylformamide (DMF) were allowed to react for 15 min at room temperature. This mixture was added to a solution of Lys^5^(BOC)-TOC in DMF and water, and the reaction was allowed to proceed for 1 h. The products of this reaction were purified on a SepPak column, and the derivative peptide was deprotected with trifluoroacetic acid containing thioanisole. The deprotected HYNIC-TOC was then purified by high-performance liquid chromatography (HPLC) (9, 10).

Radiolabeling of HYNIC-TOC was performed in an ethylenediamine diacetic acid (EDDA) solution (pH 7.0). The HYNIC-TOC was mixed with a solution of pertechnetate (^99m^TcO_4_^-^) containing tin in 0.1 N nitrogen-purged hydrochloric acid (HCl). The reaction was carried out at room temperature for 60 min, and the radiolabeled HYNIC-TOC was separated from free pertechnetate by HPLC (9, 10). The mean radiochemical yield of the reaction was 63.6% and the radiochemical purity (RCP) of the product was >98% (9, 10). The specific activity of ^99m^Tc-HYNIC-TOC was reported by the investigators to be ~37 GBq/μmol (1 Ci/μmol) (9). The labeled HYNIC-TOC was stable as an aqueous solution for at least 24 h and in human plasma for at least 4 h. In human plasma, some of the labeled peptide (amount not provided by the investigators) bound to the plasma proteins that were precipitated by acetonitrile (9).

^99m^Tc-HYNIC-TOC has also been prepared by the coligand exchange of EDDA and tricine as detailed by von Guggenberg et al. (12). For this, HYNIC-TOC was incubated with EDDA (dissolved in 0.1 N HCl), tricine (in 2.0 M phosphate buffer (pH 6.0)) and tin (dissolved in nitrogen-purged 0.1 N HCl). Pertechnetate was added to the solution and the mixture was boiled for 10 min. The RCP of the product was >90%. Specific activity of the radiochemical generated by this method was not provided by the investigators (12).

HYNIC-TOC is also available as a freeze-dried kit for labeling with ^99m^TcO_4_^-^ (8,11). To generate the kit, HYNIC-TOC was dissolved in ethanol and tin chloride in 0.1 N nitrogen-purged HCl just before use. These solutions were dispensed in a solution containing EDDA, tricine, and mannitol. The solution mixture was dispensed into glass vials and frozen immediately to <–50°C. The freeze-drying was then initiated as detailed by von Guggenberg et al. (8). Upon completion of the freeze-drying procedure, the vials were capped under vacuum and stored at 2–8°C. To radiolabel the peptide, the freeze-dried formulation was reconstituted in 0.2 M phosphate buffer in the vial (pH 6–7) and pertechnetate was added to it immediately. The mixture was then boiled for 10 min. The labeled product was analyzed by HPLC and thin-layer chromatography (TLC). A number of batches (n = 10) were prepared and evaluated for labeling over 1 year (8). All preparations yielded a product with >90% RCP as determined by HPLC and TLC. The reconstituted product labeled over a 24-h period had a RCP of >90%.

González-Vázquez et al. determined the RCP of the labeled product from the reconstituted freeze-dried kit by instant TLC on silica gel and HPLC (11). Three different mobile phases were used to determine the purity by instant TLC: 2-butanone for ^99m^TcO_4_^-^ (Rf = 1), 0.1 M sodium citrate (pH 5.0) for the ^99m^Tc-coligand and ^99m^TcO_4_^-^ (Rf = 1), and methanol:1 M ammonium acetate (1:1 v/v) for ^99m^Tc-colloid (Rf = 0). The radiolabeled peptide had Rf values of 0.0, 0.0, and 0.7–1.0, respectively, in the three mobile phases. The specific activity of the labeled product was not provided by the investigators (11). In one study, ^111^In-DPTA-OCT, prepared from a commercial kit, was used for comparison (10).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+HYNIC-TOC+in+vitro)]

The in vitro properties of ^99m^Tc-HYNIC-TOC were investigated with AR42J cells, a rat pancreatic cell line (9, 10). The labeled peptide had a dissociation constant of 2.6 nmol/L for the receptor. Rapid internalization of the labeled compound, which increased with time (5% per milligram protein at 80 min), was observed in receptor binding studies with intact cells (10). During the same period, the surface-bound activity remained at <1% per milligram protein during the same period.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+HYNIC-TOC+rodentia)]

The biodistribution of ^99m^Tc-HYNIC-TOC was investigated in nude mice bearing AR42J or HepG2 (a human hepatocellular carcinoma cell line) cell tumors (10, 13). Mice with the AR42J pancreatic cell tumors (n = 8) were studied for ^99m^Tc-HYNIC-TOC uptake between 10 and 30 days after the growth of tumors (10). Eight animals were injected with the radiolabeled peptide through the tail vein. Among these, four animals had been treated with cold HYNIC-TOC 30 min before administration of the radiochemical. A significant difference in the uptake (P < 0.05) was observed between the blocked and unblocked animals. Approximately 9.6% of the injected dose per gram tissue (% ID/g) of the label accumulated in the tumors of the unblocked animals. This value was ~1.8% ID/g for the blocked animals. Residual activity was also found in the blood (~0.28% ID/g), liver (~1.06% ID/g), gut (~1.58% ID/g), pancreas (~0.45% ID/g), and kidneys (~4.7% ID/g) of the unblocked animals. The tumor/organ ratios for the accumulation of radioactivity were 33.97, 9.11, 31.29, and 2.05 for the blood, liver, muscle, and kidneys, respectively. Compared to ^111^In-DPTA-OCT, the accumulation was comparable in the liver and the gut, approximately half in the blood and muscles, and approximately 10-fold higher in the kidneys (10).

In the second study, groups of nude mice (a subcutaneous group and an intra-liver group) (n = 3 in each group) bearing HepG2 cell tumors were injected with ^99m^Tc-HYNIC-TOC through the caudal vein and imaged at 2 h and 4.5 h after the injection (13). Accumulation of radioactivity in the tumor xenografts in both animal groups was observed. The label was retained in the kidneys and excreted through the bladder. The investigators suggested that accumulation of label in the kidneys was probably because of nonspecific uptake by the tubulus cells. This can lead to nephrotoxicity, and the investigators recommended that ^99m^Tc-HYNIC-TOC should be carefully evaluated further before use in humans (13).

The accumulation of ^99m^Tc-octreotide (http://www.chemocare.com/bio/octreotide_acetate.asp) (commercially available) and ^99m^Tc-HYNIC-TOC in rat kidneys was investigated and compared by Kopecky et al. (14). In rat kidney perfusion experiments, the investigators observed that ^99m^Tc-octreotide had a three-fold lower clearance value compared to ^99m^Tc-HYNIC-TOC. The accumulation of ^99m^Tc-HYNIC-TOC for up to 48 h in the kidneys was suggested to be primarily responsible for the renal excretion of this radiopharmaceutical. The investigators also suggested that the presence of SS receptors, differences in the tonicity levels of the kidneys, and other mechanisms were probably responsible for accumulation of the SS analogs in these organs (14).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc-HYNIC-TOC+non-primate+mammals)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc-HYNIC-TOC+non-human+primates)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc-HYNIC-TOC+humans)]

Li et al. evaluated the use and biodistribution of ^99m^Tc-HYNIC-TOC to image endocrine, non-endocrine, and benign tumors in humans (15). In this study, imaging with ^99m^Tc-HYNIC-TOC was also compared to ^111^In-pentetreotide and radioiodinated meta-[radioiodinated]iodobenzylguanidine (^131^I-MIBG) tumor imaging of the patients. The in vivo biodistribution of ^99m^Tc-HYNIC-TOC was observed to be similar to that of ^111^In-pentetreotide, with uptake primarily in the liver, spleen, and kidneys. ^99m^Tc-HYNIC-TOC imaging demonstrated intense tumor uptake at 1 hour after injection and revealed more lesions compared to ^131^I-MIBG. The investigators concluded that ^99m^Tc-HYNIC-TOC was a suitable agent for the detection of SS-positive tumors in humans (15).

In another study, the sensitivity, specificity, and accuracy of ^99m^Tc-HYNIC-TOC scintigraphy was observed to be 86.4%, 75.0%, and 84.6%, respectively, for imaging in patients with medullary thyroid carcinoma (16).

A study to compare the diagnostic efficacy of ^99m^Tc-depreotide (http://www.rxlist.com/cgi/generic/neotect.htm) and ^99m^Tc-HYNIC-TOC to differentiate between malignant and benign causes of solitary pulmonary nodules was performed in human patients (17). The investigators reported that ^99m^Tc-depreotide accumulated primarily in the spine, sternum, ribs, and lungs (mean lung/heart ratio = 2.2), but no such accumulation was observed with ^99m^Tc-EDDA/HYNIC-TOC (mean lung/heart ratio = 0.7). A comparison of scintigrams revealed ^99m^Tc-depreotide provided higher-quality images compared to ^99m^Tc-EDDA/HYNIC-TOC. In addition, ^99m^Tc-depreotide showed a higher accumulation than ^99m^Tc-EDDA/HYNIC-TOC in lung tumors compared to blood pool (heart): 4.5 ± 1.05 and 1.8 ± 0.29, respectively (P < 0.05). However, the mean tumor/lung background ratios were similar for both radiotracers (2.2 in malignant and 1.4 in benign lesions, respectively). A significantly higher non-uniformity of counts was observed with ^99m^Tc-EDDA/HYNIC-TOC compared to ^99m^Tc-depreotide (16.4% versus 11.4%; P < 0.01) in the lung background region (17).

[underlined: González-Vázquez] (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=Search&Term=%22Gonz%C3%A1lez-V%C3%A1zquez%20A%22%5BAuthor%5D&itool=EntrezSystem2.PEntrez.Pubmed.Pubmed_ResultsPanel.Pubmed_RVAbstractPlus)et al. studied the biokinetic model for ^99m^Tc-HYNIC-TOC prepared from lyophilized kits and evaluated its dosimetry as a tumor-imaging agent in patients with histologically confirmed neuroendocrine tumors (11). Whole-body images from patients were acquired between 5 min and 24 h after administration of ^99m^Tc-HYNIC-TOC. The images showed an average tumor/blood (heart) ratio of 4.3 ± 0.7 in receptor-positive tumors at 1 h. The mean absorbed radiation doses calculated for this study with the use of 740 MBq (20 mCi) of ^99m^Tc-HYNIC-TOC were 24, 21.5, 5.5, and 1.0 mSv (2.4, 2.15, 0.55, and 0.1 rem) for spleen, kidneys, liver, and bone marrow, respectively; the radiochemical had an effective dose of 4.4 mSv (0.44 rem) (11).

^99m^Tc-HYNIC-TOC scintigraphy was used to assess the retrobulbar irradiation response in Graves' ophthalmopathy (GO) patients (7). Patients were treated with octreoscan (http://www.drugs.com/pro/octreoscan.html) followed by retrobulbar irradiation therapy. The response to therapy was then assessed 3 months after start of the treatment. Of the 14 GO patients enrolled in the study, 8 (57.1%) patients responded to retrobulbar radiotherapy and 6 (42.9%) patients were non-responders. Using the orbital/occipital ratio, the 8 responders were compared to the 6 non-responders for the orbital uptake of ^99m^Tc-HYNIC-TOC. At 4 h after administration, ^99m^Tc-HYNIC-TOC scintigraphy showed that the responders had a higher (P = 0.001) orbital/occipital uptake ratio than the non-responders, and a significant correlation (P = 0.034) was observed between the orbital/occipital ratio and the clinical activity score of the study. It was also observed that the 8 patients who responded to therapy were also positive for scintigraphy, but 5 of the 6 non-responding patients were negative for scintigraphy. The investigators concluded that orbital ^99m^Tc-HYNIC-TOC scintigraphy was useful for the estimation of disease activity and for the prediction of the response to subsequent radiotherapy in GO patient, and that patients who were positive for octreoscan were more likely to respond to irradiation therapy (7).

## References

1 Hofland L.J., Lamberts S.W. (2003). The pathophysiological consequences of somatostatin receptor internalization and resistance. Endocr Rev.
2 Breeman W.A., Kwekkeboom D.J., de Blois E., de Jong M., Visser T.J., Krenning E.P. (2007). Radiolabelled regulatory peptides for imaging and therapy. Anticancer Agents Med Chem.
3 Reubi J.C. (2003). Peptide receptors as molecular targets for cancer diagnosis and therapy. Endocr Rev.
4 Forrer F., Waldherr C., Maecke H.R., Mueller-Brand J. (2006). Targeted radionuclide therapy with 90Y-DOTATOC in patients with neuroendocrine tumors. Anticancer Res.
5 Koukouraki S., Strauss L.G., Georgoulias V., Schuhmacher J., Haberkorn U., Karkavitsas N., Dimitrakopoulou-Strauss A. (2006). Evaluation of the pharmacokinetics of 68Ga-DOTATOC in patients with metastatic neuroendocrine tumours scheduled for 90Y-DOTATOC therapy. Eur J Nucl Med Mol Imaging.
6 Moody T.W., Chan D., Fahrenkrug J., Jensen R.T. (2003). Neuropeptides as autocrine growth factors in cancer cells. Curr Pharm Des.
7 Sun H., Jiang X.F., Wang S., Chen H.Y., Sun J., Li P.Y., Ning G., Zhao Y.J. (2007). 99mTc-HYNIC-TOC scintigraphy in evaluation of active Graves' ophthalmopathy (GO). Endocrine.
8 von Guggenberg E., Mikolajczak R., Janota B., Riccabona G., Decristoforo C. (2004). Radiopharmaceutical development of a freeze-dried kit formulation for the preparation of [99mTc-EDDA-HYNIC-D-phe1, Tyr3]-octreotide, a somatostatin analog for tumor diagnosis. Journal of Pharmaceutical Sciences.
9 Decristoforo C., Mather S.J. (1999). Preparation, 99mTc-labeling, and in vitro characterization of HYNIC and N3S modified RC-160 and [Tyr3]octreotide. Bioconjug Chem.
10 Decristoforo C., Melendez-Alafort L., Sosabowski J.K., Mather S.J. (2000). 99mTc-HYNIC-[Tyr3]-octreotide for imaging somatostatin-receptor-positive tumors: preclinical evaluation and comparison with 111In-octreotide. J Nucl Med.
11 Gonzalez-Vazquez A., Ferro-Flores G., Arteaga de Murphy C., Gutierrez-Garcia Z. (2006). Biokinetics and dosimetry in patients of 99mTc-EDDA/HYNIC-Tyr3-octreotide prepared from lyophilized kits. Appl Radiat Isot.
12 Von Guggenberg E., Sarg B., Lindner H., Alafort L.M., Mather S.J., Moncayo R., Decristoforo C. (2003). Preparation via coligand exchange and characterization of [99mTc-EDDA-HYNIC-D-Phen1, Tyr3]octereotide(99mTc-EDDA/HYNIC-TOC). Journal of Labelled Compounds and Radiopharmaceuticals.
13 Li Y., Si J.M., Zhang J., Du J., Wang F., Jia B. (2005). Somatostatin receptor subtype 2-mediated scintigraphy and localization using (99m)Tc-HYNIC-Tyr(3)-octreotide in human hepatocellular carcinoma-bearing nude mice. World J Gastroenterol.
14 Kopecky M., Semecky V., Trejtnar F., Laznicek M., Laznickova A., Nachtigal P., Decristoforo C., Mather S.J., Macke H.R. (2004). Analysis of accumulation of 99mTc-octreotide and 99mTc-EDDA/HYNIC-Tyr3-octreotide in the rat kidneys. Nucl Med Biol.
15 Li F., Chen L.B., Jing H.L., Du Y.R., Chen F. (2003). , and , .
16 Czepczynski R., Kosowicz J., Ziemnicka K., Mikolajczak R., Gryczynska M., Sowinski J. (2006). , and , .
17 Plachcinska A., Mikolajczak R., Kozak J., Rzeszutek K., Kusmierek J. (2006). Comparative analysis of 99mTc-depreotide and 99mTc-EDDA/HYNIC-TOC thorax scintigrams acquired for the purpose of differential diagnosis of solitary pulmonary nodules. Nucl Med Rev Cent East Eur.